# N-[[4'-[(2-Ethyl-5,7-dimethyl-3H-imidazo[4,5-b]pyridine-3-yl)methyl][1,1'-biphenyl]-2-yl]sul-fonyl]-4-[^11^C]methoxybenzamide

Chemical name: | N-[[4'-[(2-Ethyl-5,7-dimethyl-3H-imidazo[4,5-b]pyridine-3-yl)methyl][1,1'-biphenyl]-2-yl]sul-fonyl]-4-[^11^C]methoxybenzamide
Abbreviated name:
Synonym: | [^11^C]L-159,884
Agent category: | Compound
Target: | Angiotensin type 1 (AT_1_) receptor
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-Human Primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=L-159,884)]

Angiotensin II (Ang II), an octapeptide, plays an important role in the regulation of cardiovascular, renal, and endocrine functions (1, 2). Ang II induces a variety of physiologic changes, such as constriction of vascular smooth muscle cells, modulation of glomerular filtration rate, and sodium retention, resulting in an increase in blood pressure. Two subtypes of Ang II receptors, AT_1_ and AT_2_, have been well characterized pharmacologically and biochemically (3, 4). AT_1_ is indicated in all known pressor effects of Ang II, whereas no direct Ang II biological functions have been found for AT_2_. The AT_1_ receptor subtype is found mainly in all vascular tissues and the pituitary gland and is the only subtype in the liver. The AT_2_ receptor subtype is found mainly in the rat adrenal medulla, human uterus, rat ovarian granulosa cells, and rat striatum (4-6). In other tissues, such as the adrenal cortex, kidneys, heart, and brain, there is a mixture of both subtypes.

The AT_1_ nonpeptide antagonist losartan (MK-954 or DuP753) has been shown to be an effective antihypertensive agent (7). MK-996 (L-159,282), a losartan analog, was found to be a potent and selective AT_1_ antagonist with high affinity (inhibitory concentration (IC_50_) = 0.15 nM for AT_1_ and >300 nM for AT_2_) (8). L-159,884, the methoxyl analog of MK-996 (IC_50_ = 0.08 nM) (9), has been synthesized as [^11^C]L-159,884 (N-[[4´[(2-ethyl-5,7-dimethyl-3H-imidazo[4,5-b]pyridin-3-yl)methyl][1,1´-biphenyl]-2-yl]sulfonyl]-4-[^11^C]methoxybenzamide) for in vivo investigation of AT_1_ expression by positron emission tomography (PET) in the kidneys, adrenal glands, and heart.

### Related Resource Links

- Chapters in MICAD (AT_1_ (http://www.ncbi.nlm.nih.gov/books?term=AT1%20receptor%20%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (AT_1_ (http://www.ncbi.nlm.nih.gov/gene/185)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=cholinesterase) (AT_1_ (http://omim.org/entry/106165))
- Clinical trials (AT_1_ (http://www.clinicaltrials.gov/ct2/results?term=Angiotensin+II+receptor))
- Drug information in FDA (AT_1_ (http://google-test.fda.gov/search?q=Angiotensin+II+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=17&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=L-159884%20and%20synthesis)]

Hamill et al. (9) reported synthesis of [^11^C]L-159,884 by O-methylation of the corresponding desmethyl phenolic precursor with [^11^C]methyl iodide in the presence of tetrabutylammonium hydroxide in dimethylformamide. The average radiochemical yield was 5% (based on [^11^C]methyl iodide, not corrected for decay) with a total synthesis time of 18 min from end of bombardment. The average specific activity was 63 GBq/μmol (2.8 Ci/μmol at end of synthesis) with radiochemical purities >95%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=L-159884%20and%20in%20vitro)]

Hamill et al. (9) obtained an IC_50_ of 0.08 nM for L-159,884 in rabbit aorta tissue.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=L-159884%20and%20rodentia)]

Biodistribution studies in mice were performed by Kim et al. (10) and showed high accumulation of radioactivity in the liver (33.51% of injected dose (ID)/g), followed by the kidneys (5.61% ID/g), lungs (3.02% ID/g), spleen (2.36% ID/g), and heart (1.56% ID/g) at 15 min after injection of [^11^C]L-159,884. There was marked accumulation of the tracer in the liver within the first 5 min (43.85% ID/g), followed by a rapid decrease of radioactivity to 7.72% ID/g at 90 min. More than 20% of the radioactivity accumulated in the intestines at 90 min, whereas <8% was collected in the urine at 90 min, suggesting that the excretion of [^11^C]L-159,884 occurred primarily through the hepatobiliary route. The decrease of radioactivity from peak levels in other tissues was more gradual. The kidney/blood and lung/blood ratios were 4.0-6.3 and 2.2-2.5 at 30-90 min, respectively. Pretreatment with L-159,282, an AT_1_ antagonist (1 mg/kg), effectively blocked specific binding of [^11^C]L-159,884 in the kidneys, lungs, and heart. Little inhibition was seen in the liver. Three other AT_1_ antagonists blocked [^11^C]L-159,884 binding in mouse kidneys, with an order of potency similar to their ability to block Ang II binding in vivo in rats. PD 123319 (AT_2_), prazosin (α_1_), yohimbine (α_2_), and propranolol (β) had little effect on [^11^C]L-159,884 binding in mouse kidneys in vivo. [^11^C]L-159,884 thus displays selective uptake and wash-out kinetics characteristic of reversible radiotracers.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=L-159884%20and%20(pig%20or%20dog%20or%20sheep%20or%20rabbit))]

Szabo et al. (11) performed quantitative PET measurements of [^11^C]L-159,884 binding in the kidneys of six dogs, using kinetic and graphical analyses (Gjedde-Patlak) with arterial input function. The dogs received intravenous injections containing 0.47 MBq (17 mCi) of [^11^C]L-159,884. Renal accumulation and kinetics of [^11^C]L-159,884 were imaged at baseline and after pretreatment with the AT_1_ antagonist MK-996 (1 mg/kg). There was selective [^11^C]L-159,884 binding in the kidneys, mainly in the cortex. Within the time interval between 95 and 115 min after injection, the radioactivity retained in the kidneys was 109 ± 27 and 42 ± 4 nCi/ml/mCi of the injected dose for the control and MK-996 studies, respectively. The fraction of unchanged [^11^C]L-159,884 in plasma samples, as determined by high-performance liquid chromatography, was 75% at 5 min and 25% at 60 min after injection. The influx rate constant for [^11^C]L-159,884 decreased from a baseline of 0.0298 ± 0.0156 to a post-MK-996 value of 0.0098 ± 0.0052, and the binding potential decreased from a baseline of 8.65 ± 2.91 to a post-MK-996 value of 3.76 ± 2.20 (P = 0.001; n = 4).These results demonstrate distinct binding of [^11^C]L-159,884 in the renal cortex with a specific binding component suitable for quantitative PET imaging of AT_1_ receptors.

Using PET studies of [^11^C]L-159,884 in dogs, Szabo et al. (12) demonstrated that increasing dietary sodium up-regulated whereas decreasing dietary sodium down-regulated AT_1_ receptors in the kidney. Owonikoko et al. (13) demonstrated that estrogen deficiency up-regulated whereas hormone replacement down-regulated AT_1_ receptors in the kidney and adrenal glands in estrogen-deficient dogs.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=L-159884%20and%20(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=L-159884%20and%20human)]

No publication is currently available.

## NIH Support

R01 DK50183

## References

1 Ferrario C.M. (1990). The renin-angiotensin system: importance in physiology and pathology. J Cardiovasc Pharmacol.
2 Griendling K.K., Murphy T.J., Alexander R.W. (1993). Molecular biology of the renin-angiotensin system. Circulation.
3 Griendling K.K., Lassegue B., Murphy T.J., Alexander R.W. (1994). Angiotensin II receptor pharmacology. Adv Pharmacol.
4 Timmermans P.B., Chiu A.T., Herblin W.F., Wong P.C., Smith R.D. (1992). Angiotensin II receptor subtypes. Am J Hypertens.
5 Chang R.S., Lotti V.J. (1991). Angiotensin receptor subtypes in rat, rabbit and monkey tissues: relative distribution and species dependency. Life Sci.
6 Leung K.H., Smith R.D., Timmermans B.M., Chiu A.T. (1991). Regional distribution of the two subtypes of angiotensin II receptor in rat brain using selective nonpeptide antagonists. Neurosci Lett.
7 Duncia J.V., Carini D.J., Chiu A.T., Johnson A.L., Price W.A., Wong P.C., Wexler R.R., Timmermans P.B. (1992). The discovery of DuP 753, a potent, orally active nonpeptide angiotensin II receptor antagonist. Med Res Rev.
8 Chakravarty P.K., Naylor E.M., Chen A., Chang R.S., Chen T.B., Faust K.A., Lotti V.J., Kivlighn S.D., Gable R.A., Zingaro G.J., et al. (1994). A highly potent, orally active imidazo[4,5-b]pyridine biphenylacylsulfonamide (MK-996; L-159,282): a new AT1-selective angiotensin II receptor antagonist. J Med Chem.
9 Hamill T.G., Burns H.D., Dannals R.F., Mathews W.B., Musachio J.L., Ravert H.T., Naylor E.M. (1996). Development of [11C]L-159,884: a radiolabelled, nonpeptide angiotensin II antagonist that is useful for angiotensin II, AT1 receptor imaging. Appl Radiat Isot.
10 Kim S.E., Scheffel U., Szabo Z., Burns H.D., Gibson R.E., Ravert H.T., Mathews W.B., Hamill T.G., Dannals R.F. (1996). In vivo labeling of angiotensin II receptors with a carbon-11-labeled selective nonpeptide antagonist. J Nucl Med.
11 Szabo Z., Kao P.F., Burns H.D., Gibson R.E., Hamill T.G., Ravert H.T., Kim S.E., Mathews W.B., Musachio J.L., Scheffel U., Dannals R.F. (1998). Investigation of angiotensin II/AT1 receptors with carbon-11-L-159,884: a selective AT1 antagonist. J Nucl Med.
12 Szabo Z., Speth R.C., Brown P.R., Kerenyi L., Kao P.F., Mathews W.B., Ravert H.T., Hilton J., Rauseo P., Dannals R.F., Zheng W., Lee S., Sandberg K. (2001). Use of positron emission tomography to study AT1 receptor regulation in vivo. J Am Soc Nephrol.
13 Owonikoko T.K., Fabucci M.E., Brown P.R., Nisar N., Hilton J., Mathews W.B., Ravert H.T., Rauseo P., Sandberg K., Dannals R.F., Szabo Z. (2004). In vivo investigation of estrogen regulation of adrenal and renal angiotensin (AT1) receptor expression by PET. J Nucl Med.